# [^64^Cu]-1,4,7,10-Tetra-azacyclododecane-N,N’,N’’,N’’’-tetraacetic acid conjugated knottin 2.5D

Chemical name: | [^64^Cu]-1,4,7,10-Tetra-azacyclododecane-N,N’,N’’,N’’’-tetraacetic acid conjugated knottin 2.5D
Abbreviated name: | [^64^Cu]Knottin 2.5D; ^64^Cu-DOTA-2.5D
Synonym:
Agent Category: | Ligand
Target: | α_v_β_3_, α_v_β_5_, and α_5_β_1_ integrin receptors
Target Category: | Receptors
Method of detection: | Positron emission tomography (PET)
Source of signal / contrast: | ^64^Cu
Activation: | No
Studies: | - In vitro; - Rodents | Structure not available in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=knottin+peptides)]

Integrin receptors that mediate tumor angiogenesis, growth, and metastasis through a complex network of signaling pathways are known to be expressed on the surface of cancerous tumor cells and neovasculature (1-3). Because of their role in tumor development and progression, inhibition of integrin receptor activity is being actively investigated in clinical trials for the treatment (http://clinicaltrials.gov/ct2/results?term=integrin+inhibitors) and imaging (http://clinicaltrials.gov/ct2/results?term=integrin+imaging) of various cancers (4, 5). Non-invasive imaging probes can be used to determine not only the efficacy of integrin-targeted anti-cancer drugs, but also to monitor disease progression and metastasis (6, 7). Although integrin receptors usually bind through the arginine-glycine-aspartic acid (RGD) motif of the extracellular matrix protein ligands, it is the amino acid residues surrounding the RGD motif that determine the receptor specificity and affinity for the ligand (4, 8, 9). As a result of the small size of the drugs, mainly peptides, that target the integrin receptor, it has been challenging to generate peptides containing the RGD motif that have an improved pharmacokinetic behavior, receptor affinity, and tumor uptake for in vivo imaging purposes. Any modification of the peptide structure has yielded integrin-targeted imaging agents that have only a limited advancement and application in the clinics (10, 11). Only one imaging compound with an RGD motif, a radioactive fluorine-labeled cyclic pentapeptide ([^18^F]-galacto-RGD), was determined to be suitable to identify integrin-positive tumors and to investigate α_v_β_3_ integrin expression in humans. However, [^18^F]-galacto-RGD has been shown to have a low tumor uptake, and it generated a high background signal due to accumulation in the liver (12, 13).

In an effort to develop imaging agents for the detection of integrin receptors expressed on tumor cell surface and neovasculature, Kimura et al. (14) used the directed evolution technique (15, 16) to place the integrin-binding RGD motif into a cystine knot peptide (also known as knottins) trypsin inhibitor of the squash plant (Ecballium elaterium) (17). The peptide was reported to have a high affinity for the α_v_β_3_ and α_v_β_5_ or the α_v_β_3_, α_v_β_5_, and α_5_β_1_ integrin receptors. In general, knottins have a core structure containing a disulfide bond, are resistant to proteolysis, have a high thermodynamic stability, and are nonimmunogenic (14). The knottin peptide containing an RGD motif (designated as knottin 2.5D) was labeled with radioactive copper (^64^Cu) to obtain [^64^Cu]knottin 2.5D (^64^Cu-1,4,7,10-tetra-azacyclododecane-N,N’,N’’,N’’’-tetraacetic acid-2.5D (^64^Cu-DOTA-2.5D)) and used to image xenograft tumors in mice with positron emission tomography (PET). It is pertinent to mention here that the amino acid sequence and structure of knottins 2.5D and 2.5F (also studied by Kimura et. al. (14)) are discussed elsewhere (14).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=64Cu+knottin+2%2E5D+synthesis)]

The synthesis of knottin 2.5D was performed with the use of the 9-fluorenylmethylcarbonyl-based solid-phase technique as described by Kimura et al. (14). In addition, two other knottin peptides, FN-RGD2 (for use as positive a control) and FN-RDG2 (negative control) were synthesized using the same technique mentioned above. A third peptide, c(RGDyK), was obtained from commercial sources for use as a second control. The amino acid sequence, structure, and properties of the various integrin-binding peptides used for studies described in this chapter are discussed by Kimura et al. (14).

To radiolabel knottin 2.5D, the peptide was mixed with molar excess of an in situ preparation of a sulfosuccinimide ester of DOTA for 1 h at room temperature and then overnight at 4°C (14). By this reaction the chelating agent was attached at the amino terminal of the folded knottin peptide for chelation of the radionuclide (^64^Cu). The final product, a knottin 2.5D-DOTA conjugate, was purified with reverse-phase high-performance liquid chromatography (RP-HPLC) on a C_18_ column as described by Kimura et al. (14). After folding the conjugated peptide as detailed by Kimura et al. (14), the agent was purified with semi-preparative RP-HPLC and freeze-dried for storage at room temperature until required. The peptide purity and molecular mass were confirmed with analytical RP-HPLC and electrospray ionization mass spectrometery. To label with ^64^Cu, the knottin 2.5D-DOTA conjugate was incubated with ^64^CuCl_2_ in 0.1 N sodium acetate buffer (pH 6.3) for 1 h at 45°C. The reaction was terminated by the addition of ethylenediamine-tetraacetic acid, and the radiolabeled product was purified with radio-HPLC on a PD-10 column. The purified product was dried, reconstituted in phosphate-buffered saline, and sterilized by filtration. For use as controls, ^64^Cu-labeled FN-RGD2, FN-RDG2, and c(RGDyK) were also respectively synthesized using the protocol described above. The radiochemical yield of the purified products was usually >80% (at least seven reactions/purifications were performed respectively on different days), and the purity was >95% as determined with HPLC. The specific activity of the various ^64^Cu-labeled peptides was not reported.

The stability of ^64^Cu-DOTA-2.5D was determined by exposing it to mouse serum for 1, 4, and 24 h at 37°C (14). Minimal degradation of the radiolabeled peptide was reported at all the time points as determined with HPLC.

Echistatin labeled with radioactive iodine (^125^I-echistatin), used as a control in some studies, was obtained from a commercial source (14).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=64Cu+knottin+2%2E5D+in+vitro+studies)]

To determine the relative integrin-binding affinities (reported as 50% inhibitory concentration (IC_50_)) of the modified and unmodified peptides, including knottin 2.5D, a competition binding assay was performed with ^125^I-echistatin (a strong antagonist of α_v_β_3_, α_v_β_5_, α_5_β_1_ and α_iib_β_3_ integrins (14)) using U-87MG cells (a human glioblastoma cell line that expresses several types of integrins on the cell surface) as described by Kimura et al. (14). The IC_50_ for DOTA-knottin 2.5D was determined to be 19 ± 6 nmol/L compared with an IC_50_ values of 370 ± 150 nmol/L and 860 ± 400 nmol/L for the control DOTA-conjugated FN-RGD2 and c(RGDyK) peptides, respectively. The negative control peptide, DOTA-FN-RDG2, did not compete with ^125^I-echistatin for binding to the U-87MG cells. The DOTA-conjugated peptides (modified) were reported to have IC_50_ values comparable to the unmodified peptides (14).

The integrin-binding specificity of the DOTA-conjugated knottin peptides was investigated with a competition assay using ^125^I-echistatin (14). Different concentrations (5 and 50 nmol/L) of the unlabeled DOTA-conjugated knottin peptides were respectively incubated with ^125^I-echistatin in microtiter plates coated with detergent-solubalized α_v_β_3_, α_v_β_5_, α_5_β_1_, and α_iib_β_3_ integrin receptors for 3 h at room temperature. The plates were washed three times to remove unbound radioactivity, and the contents were solubalized in 2 N sodium hydroxide to determine the amount of receptor-bound radioactivity. Compared with the FN-RGD2 and c(RGDyK) peptides, the knottin 2.5D peptide exhibited a higher binding (fro details see Figure 2A in reference 14) to the different integrins receptors except α_iib_β_3_, which is expressed mainly on the platelet cells (14).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=64Cu+knottin+2%2E5D+rodentia)]

The use of ^64^Cu-DOTA-2.5D as a PET imaging probe was investigated in mice bearing human U-87MG cell xenograft tumors (14). The animals (n = 3 or more for each probe) were injected with the respective ^64^Cu-DOTA-conjugated peptides through the tail vein and imaged 1 h later for up to 24 h. Calibration of the PET images for quantitation purposes was done as described by Wu et. al (18). At 1 h after administration of the labeled peptides, the tumor uptake of ^64^Cu-DOTA-2.5D was higher (4.47 ± 1.21% injected dose/gram tissue (% ID/g)) compared with the control ^64^Cu-DOTA-FN-RGD2 (1.48 ± 0.53% ID/g) and ^64^Cu-DOTA-c(RGDyK) (2.32 ± 0.55% ID/g) peptides. Also, compared with ^64^Cu-DOTA-FN-RGD2 (4.19 ± 0.78% ID/g and 3.59 ± 0.87% ID/g at 1 and 4 h after injection, respectively), a lower uptake of ^64^Cu-DOTA-2.5D (~2% ID/g) was observed in the liver. Coinjection of ^64^Cu-DOTA-2.5D with molar excess (0.5 μmol) of unlabeled DOTA-c(RGDyK) was reported to block tumor uptake (1.67 ± 0.28% ID/g) of radioactivity at 1 h after administration of the labeled peptide. For the negative control peptide, ^64^Cu-DOTA-FN-RDG2, the tumor accumulation of radioactivity was reported to be 1.09 ± 0.48% ID/g and 0.76 ± 0.33% ID/g at 1 and 4 h after injection, respectively.

For the in vivo biodistribution studies, animals bearing U-87MG cell xenograft tumors (at least three mice per time point) were injected with ^64^Cu-knottin 2.5D through the tail vein, and the amount of radioactivity accumulated in the major organs was determined after 0.5 and 4 h (14). At 0.5 h, varying amounts of radioactivity (1.5–8.0% ID/g) were detected primarily in the tumor, blood, liver, lungs, kidneys, spleen, intestines, skin, and the stomach (for details see Figure 4C in reference 14). By 4 h after administration, the radioactivity was reduced to between <1% ID/g (liver, lung, spleen, intestines, skin, and stomach) and ~2% ID/g (liver) and ~3% ID/g (kidneys).

From these studies the investigators concluded that the direct evolution–engineered integrin-binding peptides had a good potential for the detection and diagnosis of various cancers (14).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22%20SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=64Cu+knottin+2%2E5D+Non+Human+Primates)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=64Cu+knottin+2%2E5D+Human+Studies)]

No references are currently available.

## Supplemental Information

[Disclaimers]

## NIH Support

Some of the work presented in this chapter was supported by National Cancer Institute grants 5K01 CA104706, 5R25T CA118681, and R25T CA118681 and a National Institutes of Health grant P50 CA114747.

## References

1 Legate K.R., Wickstrom S.A., Fassler R. (2009). Genetic and cell biological analysis of integrin outside-in signaling. Genes Dev.
2 Pontier S.M., Muller W.J. (2009). Integrins in mammary-stem-cell biology and breast-cancer progression--a role in cancer stem cells?. J Cell Sci.
3 Streuli C.H. (2009). Integrins and cell-fate determination. J Cell Sci.
4 Moschos S.J., Drogowski L.M., Reppert S.L., Kirkwood J.M. (2007). Integrins and cancer. Oncology.
5 Fujita Y., Abe R., Shimizu H. (2008). Clinical approaches toward tumor angiogenesis: past, present and future. Curr Pharm Des.
6 Zaccaro L., Del Gatto A., Pedone C., Saviano M. (2009). Peptides for tumour therapy and diagnosis: current status and future directions. Curr Med Chem.
7 Haubner R., Decristoforo C. (2009). Radiolabelled RGD peptides and peptidomimetics for tumour targeting. Front Biosci.
8 Chen, C.Y., J.H. Shiu, Y.H. Hsieh, Y.C. Liu, Y.C. Chen, Y.C. Chen, W.Y. Jeng, M.J. Tang, S.J. Lo, and W.J. Chuang, Effect of D to E mutation of the RGD motif in rhodostomin on its activity, structure, and dynamics: Importance of the interactions between the D residue and integrin. Proteins, 2009
9 Manzoni, L., L. Belvisi, D. Arosio, M. Civera, M. Pilkington-Miksa, D. Potenza, A. Caprini, E.M. Araldi, E. Monferini, M. Mancino, F. Podesta, and C. Scolastico, Cyclic RGD-Containing Functionalized Azabicycloalkane Peptides as Potent Integrin Antagonists for Tumor Targeting. ChemMedChem, 2009
10 Cai W., Rao J., Gambhir S.S., Chen X. (2006). How molecular imaging is speeding up antiangiogenic drug development. Mol Cancer Ther.
11 Haubner R. (2006). Alphavbeta3-integrin imaging: a new approach to characterise angiogenesis?. Eur J Nucl Med Mol Imaging.
12 Haubner R., Weber W.A., Beer A.J., Vabuliene E., Reim D., Sarbia M., Becker K.F., Goebel M., Hein R., Wester H.J., Kessler H., Schwaiger M. (2005). Noninvasive visualization of the activated alphavbeta3 integrin in cancer patients by positron emission tomography and [18F]Galacto-RGD. PLoS Med.
13 Beer A.J., Haubner R., Sarbia M., Goebel M., Luderschmidt S., Grosu A.L., Schnell O., Niemeyer M., Kessler H., Wester H.J., Weber W.A., Schwaiger M. (2006). Positron emission tomography using [18F]Galacto-RGD identifies the level of integrin alpha(v)beta3 expression in man. Clin Cancer Res.
14 Kimura R.H., Cheng Z., Gambhir S.S., Cochran J.R. (2009). Engineered knottin peptides: a new class of agents for imaging integrin expression in living subjects. Cancer Res.
15 Otten L.G., Quax W.J. (2005). Directed evolution: selecting today's biocatalysts. Biomol Eng.
16 Leemhuis H., Kelly R.M., Dijkhuizen L. (2009). Directed evolution of enzymes: Library screening strategies. IUBMB Life.
17 Favel A., Mattras H., Coletti-Previero M.A., Zwilling R., Robinson E.A., Castro B. (1989). Protease inhibitors from Ecballium elaterium seeds. Int J Pept Protein Res.
18 Wu Y., Zhang X., Xiong Z., Cheng Z., Fisher D.R., Liu S., Gambhir S.S., Chen X. (2005). microPET imaging of glioma integrin {alpha}v{beta}3 expression using (64)Cu-labeled tetrameric RGD peptide. J Nucl Med.